# Gadolinium-anti-neutrophil gelatinase-associated lipocalin 2 24p3 antibody-conjugated micelles

Chemical name: | Gadolinium-anti-neutrophil gelatinase-associated lipocalin 2 24p3 antibody-conjugated micelles
Abbreviated name: | NGAL/24p3-Targeted micelles
Synonym:
Agent category: | Antibody
Target: | Neutrophil gelatinase-associated lipocalin 2 (NGAL, 24p3)
Target category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAD37404.1) and gene (http://www.ncbi.nlm.nih.gov/gene/4318) for more information about MMP-9.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=24P3%20micelles)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play an important role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degradation of the basement membrane and ECM (3). Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (4-7).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (8, 9). Gd-diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous magnetic resonance imaging (MRI) contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and in cancerous tissues. Various macromolecular Gd complexes have demonstrated superior contrast enhancement for MRI of the vasculature and carcinomas (10-12); however, these Gd complexes cannot proceed into further clinical development because of high tissue accumulation and slow excretion of toxic Gd ions. Furthermore, they are largely nonspecific.

Mouse 24p3 protein is a member of the lipocalin family of proteins (13). The protein is considered a homolog of human neutrophil gelatinase MMP-9–associated lipocalin-2 (NGAL), a multifunctional protein identified originally by Kjeldsen et al. (14). NGAL/24p3 protein is also released by macrophages, prolonging the activity of MMPs and destabilizing atherosclerotic plaques (15). In this chapter, a rat anti-mouse 24p3 monoclonal antibody (MAB1857) was incorporated into di-stearoyl-polyethylene glycol-phosphatidylethanolamine 2000 (DSPE-PEG2000) micelles labeled with Gd for use in MRI of vulnerable atherosclerotic plaques (16, 17).

### Related Resource Links:

- Chapters in MICAD (MMPs (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=MMP+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Lipocalin-2 (http://www.ncbi.nlm.nih.gov/gene/3934), MMP-9 (http://www.ncbi.nlm.nih.gov/gene/4318))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Lipocalin-2 (http://www.ncbi.nlm.nih.gov/omim/600181), MMP-9 (http://www.ncbi.nlm.nih.gov/omim/120361))
- Clinical trials (Lipocalin-2 (http://www.clinicaltrials.gov/ct2/results?term=Lipocalin-2), MMP-9 (http://www.clinicaltrials.gov/ct2/results?term=MMP-9))
- Drug information in FDA (Lipocalin-2 (http://google2.fda.gov/search?q=Lipocalin-2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=13), MMP-9 (http://google2.fda.gov/search?q=mmp-9&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=11))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=24P3%20micelles+synthesis)]

A mixture of DSPE-PEG2000, Gd-DTPA-bis-stearylamide, lissamine-rhodamine-phosphatidylethanolamine, and maleimide-PEG2000-DSPE in a molar ratio of 43:50:5:2 in chloroform was dried by rotary evaporation for 3 min at 40°C (17). The lipid film was subsequently hydrated with 1 ml phosphate-buffered saline for 5 min to a final lipid concentration of 10 mM. Sulfhydryl groups were added to rat anti-mouse 24p3 antibody or rat anti-mouse isotype antibody (10 mg) by incubation for 30 min at room temperature with N-succinimidyl S-acetylthioacetate. The modified antibody was added to the micelles and incubated for 14 h at 4°C. NGAL/24p3-Targeted and control micelles were purified with column chromatography. The ratio of antibody to lipid (µmol/µmol) was 0.7:100. There was ~1 antibody molecule per micelle. The size of the micelles was determined with dynamic light scattering to be 23.0 ± 1.0 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=24P3%20micelles+in+vitro)]

The control antibody micelles exhibited an r1 relaxivity value of 3.0 mM^-1^s^-1^ in phosphate-buffered saline at 9.4 T and 37°C, whereas Gd-DTPA exhibited the an r1 relaxivity value of 1.8 mM^-1^s^-1^ (17). MRI images of 24p3-coated tubes showed that NGAL/24p3-targeted micelles bound to 24p3, whereas control antibody micelles showed little binding to 24p3. No blocking study was performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=24P3%20micelles+rodentia)]

te Boekhorst et al. (16) used a 9.4-T MRI scanner to perform in vivo MRI in ApoE^-/-^/eNOS^-/-^ mice (n = 9), which exhibit severe atherosclerosis in the abdominal area. Injection of NGAL/24p3-targeted micelles (600 nmol) provided stronger enhancement in MRI contrast than control antibody micelles in the atherosclerotic aortic wall at 72 h after injection. The normalized enhancement ratios were 1.67 ± 0.12 and 1.21 ± 0.06 for NGAL/24p3-targeted micelles and control antibody micelles (P < 0.05), respectively. Immunohistochemical staining showed that NGAL/24p3-targeted micelles were colocalized with NGAL/24p3 expression and macrophages in the plaque. No blocking studies were performed to assess specificity of NGAL/24p3-targeted micelles though control antibody micelles were studied.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=24P3%20micelles+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=24P3%20micelles+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=24P3%20micelles+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
9 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
10 Schmiedl U., Ogan M., Paajanen H., Marotti M., Crooks L.E., Brito A.C., Brasch R.C. (1987). Albumin labeled with Gd-DTPA as an intravascular, blood pool-enhancing agent for MR imaging: biodistribution and imaging studies. Radiology.
11 Gossmann A., Okuhata Y., Shames D.M., Helbich T.H., Roberts T.P., Wendland M.F., Huber S., Brasch R.C. (1999). Prostate cancer tumor grade differentiation with dynamic contrast-enhanced MR imaging in the rat: comparison of macromolecular and small-molecular contrast media--preliminary experience. Radiology.
12 Preda A., van Vliet M., Krestin G.P., Brasch R.C., van Dijke C.F. (2006). Magnetic resonance macromolecular agents for monitoring tumor microvessels and angiogenesis inhibition. Invest Radiol.
13 Kjeldsen L., Cowland J.B., Borregaard N. (2000). Human neutrophil gelatinase-associated lipocalin and homologous proteins in rat and mouse. Biochim Biophys Acta.
14 Kjeldsen L., Johnsen A.H., Sengelov H., Borregaard N. (1993). Isolation and primary structure of NGAL, a novel protein associated with human neutrophil gelatinase. J Biol Chem.
15 Yan L., Borregaard N., Kjeldsen L., Moses M.A. (2001). The high molecular weight urinary matrix metalloproteinase (MMP) activity is a complex of gelatinase B/MMP-9 and neutrophil gelatinase-associated lipocalin (NGAL). Modulation of MMP-9 activity by NGAL. J Biol Chem.
16 Te Boekhorst, B.C., S.M. Bovens, W.E. Hellings, P.H. van der Kraak, K.W. van de Kolk, A. Vink, F.L. Moll, M.F. van Oosterhout, J.P. de Vries, P.A. Doevendans, M.J. Goumans, D.P. de Kleijn, C.J. van Echteld, G. Pasterkamp, and J.P. Sluijter, Molecular MRI of murine atherosclerotic plaque targeting NGAL: a protein associated with unstable human plaque characteristics. Cardiovasc Res, 2010
17 te Boekhorst B.C., Bovens S.M., Rodrigues-Feo J., Sanders H.M., van de Kolk C.W., de Kroon A.I., Cramer M.J., Doevendans P.A., ten Hove M., Pasterkamp G., van Echteld C.J. (2010). Characterization and in vitro and in vivo testing of CB2-receptor- and NGAL-targeted paramagnetic micelles for molecular MRI of vulnerable atherosclerotic plaque. Mol Imaging Biol.